# ^18^F-Tetrazine-trans-cyclooctene-Cys^40^-exendin-4

Chemical name: | ^18^F-Tetrazine-trans-cyclooctene-Cys^40^-exendin-4
Abbreviated name: | ^18^F-TTCO-Cys^40^-exendin-4
Synonym:
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis. It inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, it induces insulin release from pancreatic β-cells as well as their proliferation. The GLP-1 receptor (GLP-1R) has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1R density is considerably greater, and the GLP-1R is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1 receptor agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. Exenatide, a synthetic version of exendin-4, is the first GLP-1 mimetic approved by the United States Food and Drug Administration (FDA) for use in select patients with type 2 diabetes (5). ^68^Ga- and ^64^Cu-labled exendin-4 have been evaluated for use with positron emission tomography (PET) imaging of the GLP-1R in the β-cells in the pancreatic islets (6). However, high kidney accumulation of these radiometal tracers may hinder the imaging of the pancreas (7). Wu et al. (8) developed ^18^F-labeled exendin-4 (^18^F-tetrazine-trans-cyclooctene-Cys^40^-exendin-4 (^18^F-TTCO-Cys^40^-exendin-4)) and investigated its biodistribution in nude mice bearing subcutaneous rat insulinoma INS-1 tumors (overexpresses GLP-1R). The probe was also evaluated for the PET visualization of INS-1 tumors and islets transplanted into the mouse liver.

### Related Resource Links:

- Chapters in MICAD (GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D), exendin-4 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=exendin-4%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GLP-1R (http://omim.org/entry/138032))
- Clinical trials (exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20synthesis)]

The structure and composition of tetrazine-Cys^40^-exendin-4 were verified with high-performance liquid chromatography (HPLC) and matrix-assisted laser desorption-ionization mass spectrometry (8). ^18^F-trans-Cyclooctene (^18^F-TCO) was prepared as previously described. ^18^F-TTCO-Cys^40^-exendin-4 was prepared by incubation of 74 MBq (2 mCi) ^18^F-TCO and tetrazine-Cys^40^-exendin-4 (0.84 nmol) for 5 min at room temperature. ^18^F-TTCO-Cys^40^-exendin-4 was purified with HPLC, with >80% yield and >99% radiochemical purity (n = 4). The total synthesis time was ~90 min from the end of bombardment. The specific activity of ^18^F-TTCO-Cys^40^-exendin-4 was 13 GBq/µmol (350 mCi/µmol) at the end of synthesis. ^18^F-TTCO-Cys^40^-exendin-4 exhibited a log P value of −0.14 ± 0.03 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20in%20vitro)]

Wu et al. (8) reported that ^18^F-TTCO-Cys^40^-exendin-4 and exendin-4 demonstrated similar binding of ^125^I-exendin(9-39) to GLP-1R–positive INS-1 rat insulinoma cells, with IC_50_ values of 1.17 ± 0.34 nM and 0.76 ± 0.19 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20rodentia)]

Wu et al. (8) performed PET imaging studies at 0.5, 1, 3, and 5 h in nude mice (n = 3) bearing INS-1 tumors after intravenous injection of 3.7 MBq (0.1 mCi) ^18^F-TTCO-Cys^40^-exendin-4. The INS-1 tumors were clearly visualized, with high radioactivity accumulation of 12.8%, 13.3%, 16.0%, and 13.0% injected dose/gram (ID/g) at 0.5, 1, 3, and 5 h, respectively. Kidney radioactivity was 38.2% ID/g at 0.5 h, 22.4% ID/g at 1 h, and 8.4% ID/g at 5 h. Kidney radioactivity was lower than that reported with ^64^Cu-DO3A-VS-Cys^40^-exendin-4 (http://www.ncbi.nlm.nih.gov/books/NBK84552/) at 4 h after injection (79.7% ID/g) (7). The tumor/muscle, tumor/liver, and tumor/kidney ratios at 5 h were 14.0, 4.0, and 1.6, respectively. Co-injection with excess exendin-4 decreased the tumor radioactivity by 77%, 82%, 88%, and 88% at 0.5, 1, 3, and 5 h, respectively. Little inhibition was observed in the kidneys.

Wu et al. (8) performed PET imaging studies at 0.5, 1, 2, and 4 h in nude mice (n = 3) transplanted with 1,000 IEQ human islets in their livers after intravenous injection of 3.7 MBq (0.1 mCi) ^18^F-TTCO-Cys^40^-exendin-4. Radioactivity levels in the livers of mice transplanted with 1,000 islets (8.25%, 7.19%, 6.29%, and 5.17% ID/g at 0.5, 1, 2, and 4 h, respectively) were significantly higher than those in sham-operated control mice (4.37%, 3.52%, 2.85%, and 1.80% ID/g at 0.5, 1, 2, and 4 h, respectively) (P < 0.01) . Ex vivo autoradiography showed the localization of radioactivity to the human islet grafts (insulin-positive cells) in the mouse liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TTCO-Cys40-exendin-4%20and%20human)

No publication is currently available.

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Nielsen L.L., Young A.A., Parkes D.G. (2004). Pharmacology of exenatide (synthetic exendin-4): a potential therapeutic for improved glycemic control of type 2 diabetes. Regul Pept.
6 Wild D., Wicki A., Mansi R., Behe M., Keil B., Bernhardt P., Christofori G., Ell P.J., Macke H.R. (2010). Exendin-4-based radiopharmaceuticals for glucagonlike peptide-1 receptor PET/CT and SPECT/CT. J Nucl Med.
7 Wu Z., Todorov I., Li L., Bading J.R., Li Z., Nair I., Ishiyama K., Colcher D., Conti P.E., Fraser S.E., Shively J.E., Kandeel F. (2011). In vivo imaging of transplanted islets with 64Cu-DO3A-VS-Cys40-Exendin-4 by targeting GLP-1 receptor. Bioconjug Chem.
8 Wu Z., Liu S., Hassink M., Nair I., Park R., Li L., Todorov I., Fox J.M., Li Z., Shively J.E., Conti P.S., Kandeel F. (2013). Development and Evaluation of 18F-TTCO-Cys40-Exendin-4: A PET Probe for Imaging Transplanted Islets. J Nucl Med.